# 3-Chloro-4-[^18^F]fluorophenyl-(4-fluoro-4-[[((5-methyl-4-methylamino-pyridin-2-ylmethyl)-amino]-methyl]-piperidin-1-yl)methanone (F13714)

Chemical name: | 3-Chloro-4-[^18^F]fluorophenyl-(4-fluoro-4-[[((5-methyl-4-methylamino-pyridin-2-ylmethyl)-amino]-methyl]-piperidin-1-yl)methanone (F13714)
Abbreviated name: | [^18^F]F13714
Synonym:
Agent category: | Compound
Target: | 5-HT_1A_ serotonin receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F13714)]

5-Hydroxytryptamine (5-HT), commonly known as serotonin, has diverse physiological roles as a neurotransmitter in the central nervous system (1). 5-HT is involved in regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, schizophrenia, and obsessive-compulsive disorder (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are five receptor subtypes within the G-protein–coupled 5-HT_1_ receptor family: 5-HT_1A_, 5-HT_1B_, 5-HT_1D_, 5-HT_1E_, and 5-HT_1F_.

5-HT_1A_ receptors are abundantly present in the hippocampus, entorhinal cortex, frontal cortex, raphe nucleus, and septum; the lowest densities are observed in the basal ganglia, substantia nigra, and cerebellum (5). Some thalamic and hypothalamic nuclei have intermediate densities. 5-HT_1A_ receptors are involved in the mediation of emotion and the function of the hypothalamus. 5-HT_1A_ receptors are implicated in anxiety, depression, hallucinogenic behavior, motion sickness, and eating disorders (6). Thus, there is a need for selective ligands to investigate the pharmacological role of 5-HT_1A_ receptors.

There have been several studies to develop specific 5-HT_1A_ radioligands [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-HT1a%5BAll%20Fields%5D%20AND%20imaging%5BAll%20Fields%5D)] for positron emission tomography (PET) imaging, such as [carbonyl-^11^C]WAY 100635 (http://www.ncbi.nlm.nih.gov/books/NBK23263/), [^18^F]FPWAY (http://www.ncbi.nlm.nih.gov/books/NBK23137/), and [^18^F]MPPF (http://www.ncbi.nlm.nih.gov/books/NBK23391/). However, none of these antagonists distinguishes between the high- and low-affinity states of the 5-HT_1A_ receptors. The high-affinity state of the receptor is coupled to G-proteins, which mediate cell functions by providing intracellular signals. 2-(4-(4-(2-Methoxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazine-3,5(2H,4H)dione (MMP) was reported to be a potent agonist of 5-HT_1A_ receptors (K_i_ = 0.15 nM) (7). This led to the development of [O-methyl-^11^C]MMP ([^11^C]MMP (http://www.ncbi.nlm.nih.gov/books/NBK23229/), also known as [^11^C]CUMI-101) as a useful tool for in vivo PET imaging of the 5-HT_1A_ receptor (8-10). However, [^11^C]CUMI-101 was shown to be a partial 5-HT_1A_ agonist and therefore was less efficient in mediating cell function (11, 12). 3-Chloro-4-[^18^F]fluorophenyl-(4-fluoro-4-[[((5-methyl-4-methylamino-pyridin-2-ylmethyl)-amino]-methyl]-piperidin-1-yl)methanone ([^18^F]F13714) was evaluated as a PET probe for the 5-HT_1A_ receptor because unlabeled F13714 was found to be a selective 5-HT_1A_ agonist with subnanomolar affinity for the 5-HT_1A_ receptor (13).

### Related Resource Links:

- Chapters in MICAD (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT1A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/gene/3350))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/omim/109760))
- Clinical trials (5-HT_1A_ (http://www.clinicaltrials.gov/ct2/results?term=5-HT1A))
- Drug information in Food and Drug Administration (5-HT_1A_ (http://google2.fda.gov/search?q=5-HT1a&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F13714%20and%20synthesis)]

The automated radiosynthesis of [^18^F]F13714, reported by Lemoine et al. (13), involved standard fluoronucleophilic substitution of the corresponding nitro precursor with K[^18^F]F/Kryptofix2.2.2 in dimethyl sulfoxide for 10 min at 150°C in an automated radiosynthesis unit, followed by solid-phase extraction with a C18 cartridge. The reported overall radiochemical yield of the radiosynthesis was ~10%, the specific radioactivity was 80–150 MBq/nmol (2.16–4.10 mCi/nmol) at the end of synthesis (EOS), and the radiochemical purity was >98%. The total synthesis time was 90 min. The log D (octanol-water partition coefficient) was 2.2 (lipophilic).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F13714%20and%20in%20vitro)]

Lemoine et al. (13) performed in vitro autoradiography with [^18^F]F13714 in rat brains, which showed radioactivity in the cingulate, entorhinal cortex, hippocampus, raphe nucleus, and brain stem. Little radioactivity was observed in the cerebellum. The hippocampus/cerebellum and raphe/cerebellum ratios were 5.5 and 3.3, respectively. Competition binding studies of F13714, WAY100635, and 5-HT with [^18^F]F13714 in rat hippocampus sections were also performed. F13714 reduced the binding of [^18^F]F13714 by 28%, 77%, and 85% at 1, 10, and 100 nM F13714, respectively. WAY100635 inhibited the binding by 20%, 66%, and 83% at 1, 10, and 100 nM WAY100635, respectively. 5-HT inhibited the binding by 20%, 30%, and 70% at 1, 10, and 100 nM, respectively. Gpp(NH)p (10 µM, a non-hydrolysable analog of guanosine 5'-triphosphate) inhibited the [^18^F]F13714 binding by 70% in the cortex and 60% in the hippocampus.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F13714%20and%20rodentia)]

Ex vivo stability studies (n = 3/group) of [^18^F]F13714 in rat brain hippocampus were performed after intravenous injection of 55.5 MBq (1.5 mCi) [^18^F]F13714 (13). [^18^F]F13714 remained 80%, 90%, 94%, and 91% intact in the hippocampus at 10, 20, 30, and 40 min after injection, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F13714%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

Lemoine et al. (13) performed in vivo PET imaging studies in the brains of two male cats for 90 min after injection of 74 MBq (2 mCi) [^18^F]F13714. High radioactivity levels were observed in the hippocampus, cingulate cortex, and amygdala. The cingulate cortex/cerebellum, amygdala/cerebellum, and hippocampus/cerebellum ratios were 1.5, 1.4, and 1.2, respectively. Pretreatment with WAY100635 (1 mg/kg, 30 min) decreased the cingulate cortex/cerebellum, amygdala/cerebellum, and hippocampus/cerebellum ratios to 1.2, 12, and 1.0, respectively.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F13714%20and%20nonhuman%20primate)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F13714%20and%20human)]

No publication is currently available.

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Pazos A., Probst A., Palacios J.M. (1987). Serotonin receptors in the human brain--III. Autoradiographic mapping of serotonin-1 receptors. Neuroscience.
6 Cowen P.J. (2000). Psychopharmacology of 5-HT(1A) receptors. Nucl Med Biol.
7 Kumar J.S., Prabhakaran J., Majo V.J., Milak M.S., Hsiung S.C., Tamir H., Simpson N.R., Van Heertum R.L., Mann J.J., Parsey R.V. (2007). Synthesis and in vivo evaluation of a novel 5-HT(1A) receptor agonist radioligand [O-methyl- (11)C]2-(4-(4-(2-methoxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazi ne-3,5(2H,4H)dione in nonhuman primates. Eur J Nucl Med Mol Imaging.
8 Milak M.S., Severance A.J., Prabhakaran J., Kumar J.S., Majo V.J., Ogden R.T., Mann J.J., Parsey R.V. (2011). In vivo serotonin-sensitive binding of [11C]CUMI-101: a serotonin 1A receptor agonist positron emission tomography radiotracer. J Cereb Blood Flow Metab.
9 Hines C.S., Liow J.S., Zanotti-Fregonara P., Hirvonen J., Morse C., Pike V.W., Innis R.B. (2011). Human biodistribution and dosimetry of (1)(1)C-CUMI-101, an agonist radioligand for serotonin-1a receptors in brain. PLoS One.
10 Milak M.S., DeLorenzo C., Zanderigo F., Prabhakaran J., Kumar J.S., Majo V.J., Mann J.J., Parsey R.V. (2010). In vivo quantification of human serotonin 1A receptor using 11C-CUMI-101, an agonist PET radiotracer. J Nucl Med.
11 Hendry N., Christie I., Rabiner E.A., Laruelle M., Watson J. (2011). In vitro assessment of the agonist properties of the novel 5-HT1A receptor ligand, CUMI-101 (MMP), in rat brain tissue. Nucl Med Biol.
12 Palner M., Underwood M.D., Kumar D.J., Arango V., Knudsen G.M., John Mann J., Parsey R.V. (2011). Ex vivo evaluation of the serotonin 1A receptor partial agonist [(3)H]CUMI-101 in awake rats. Synapse.
13 Lemoine L., Becker G., Vacher B., Billard T., Lancelot S., Newman-Tancredi A., Zimmer L. (2012). Radiosynthesis and Preclinical Evaluation of 18F-F13714 as a Fluorinated 5-HT1A Receptor Agonist Radioligand for PET Neuroimaging. J Nucl Med.